# [^11^C]2-(2-[2-Dimethylaminothiazol-5-yl]ethenyl)-6-(2-[fluoro]ethoxy)benzoxazole

Chemical name: | [^11^C]2-(2-[2-Dimethylaminothiazol-5-yl]ethenyl)-6-(2-[fluoro]ethoxy)benzoxazole
Abbreviated name: | [^11^C]BF-227
Synonym:
Agent Category: | Compound
Target: | Aggregates of ß-amyloid (Aß) peptides
Target Category: | Acceptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BF-227)]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1). It is characterized pathologically by neuronal loss with the presence in the brain of senile plaques of β-amyloid (Aβ) peptides and intracellular neurofibrillary tangles of filaments that contain the hyperphosphorylated protein tau (2, 3). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD.

Early diagnosis of AD is important for treatment consideration and disease management (4). Several radioligands for positron emission tomography (PET) have been developed (5-7) and tested in humans as in vivo diagnostic tools for imaging and measuring the formation of Aβ deposits (7). The first agent successfully used in human studies was [^18^F]FDDNP (8), a malonitrile derivative found to bind to both neurofibrillary tangles and Aβ plaques. The second successful attempt was made with [^11^C]PIB (9), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1, which showed marked retention in areas of the cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand successfully tested in humans was [^11^C]4-N-methylamino-4´-hydroxystilbene ([^11^C]SB-13), a stilbene derivative that exhibits good binding affinities for Aβ aggregates in vitro, moderate lipophilicity, high initial brain uptake in the normal rat cortex, and a rapid washout (10).

Benzoxazole derivatives have shown very good binding affinities for Aβ aggregates and Aβ plaques, as well as good brain penetration (11). An optimized derivative, [^11^C]2-(2-[2-dimethylaminothiazol-5-yl]ethenyl)-6-(2-[fluoro]ethoxy)benzoxazole ([^11^C]BF-227), has been synthesized and is currently being studied as a PET radioligand for Aβ plaques (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BF-227%20and%20synthesis)]

[^11^C]BF-227 was synthesized from its precursor by N-methylation in dimethyl sulfoxide by use of ^11^C-methyl triflate (12). [^11^C]BF-227 was purified by reverse-phase high-performance liquid chromatography and solid-phase extraction with >95% radiochemical purity. The radiochemical yields on the basis of [^11^C]methyl triflate were >50% , and the specific activities were 119–138 GBq/µmol (3.2–3.7 Ci/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BF-227%20and%20in%20vitro)]

BF-227 was found to compete well with [^125^I]BF-180, a ligand selective for Aβ plaques (12). Studies of binding to Aβ1–42 fibrils in solution showed an inhibition constant (K_i_) value of 4.3 ± 1.5 nM. BF-227 exhibited a moderate lipophilicity (log P value of 1.75 at pH 7.4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BF-227%20and%20rodentia)]

Kudo et al. (12) performed in vivo biodistribution studies in normal male C57B6 mice injected intravenously with a saline solution of [^11^C]BF-227. Results showed that the radiotracer easily penetrated the blood–brain barrier, and a peak of the brain uptake of 7.9% injected dose/g (% ID/g) was observed at 2 min after injection. This value compared well with [^125^I]6-iodo-2-(4´-dimethylamino)-phenyl-imidazo[1,2-a]pyridine ([^125^I]IMPY) (7.2% ID/g at 2 min). Accumulation in the brain was 3.7% ID/g at 10 min, 1.4% ID/g at 30 min, and 0.64% ID/g at 60 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BF-227%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BF-227%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BF-227%20and%20human)]

The first human study with [^11^C]BF-227 in 10 patients with probable AD and 11 healthy control subjects was reported. Subjects were given an intravenous injection of 211–366 MBq (5.7–9.9 mCi) of [^11^C]BF-227 (12). Dynamic PET images showed that [^11^C]BF-227 retention (measured as the ratio of regional standard uptake value [SUV] to cerebellar SUV) is significantly higher in brain regions that are known to contain Aβ plaques in AD patients (e.g., the frontal, lateral temporal, parietal, temporooccipital, occipital, anterior and posterior cingulate cortices, and striatum) than in control subjects. The lateral temporal cortex SUV ratio showed no overlap between AD patients and normal control subjects. There was a similar retention of [^11^C]BF-227 in the medial temporal cortex, thalamus, cerebellum, and white matter that contained few Aβ deposits in AD patients and control subjects. No significant difference was observed in any brain regions between young normal (n = 3) and aged normal subjects (n = 8).

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
3 Brandt R., Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
4 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
5 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
6 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
7 Wu C., Pike V.W., Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
8 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
9 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Ono M., Wilson A., Nobrega J., Westaway D., Verhoeff P., Zhuang Z.P., Kung M.P., Kung H.F. (2003). 11C-labeled stilbene derivatives as Abeta-aggregate-specific PET imaging agents for Alzheimer's disease. Nucl Med Biol.
11 Kudo Y. (2006). Development of amyloid imaging PET probes for an early diagnosis of Alzheimer's disease. Minim Invasive Ther Allied Technol.
12 Kudo Y., Okamura N., Furumoto S., Tashiro M., Furukawa K., Maruyama M., Itoh M., Iwata R., Yanai K., Arai H. (2007). 2-(2-[2-Dimethylaminothiazol-5-yl]Ethenyl)-6- (2-[Fluoro]Ethoxy)Benzoxazole: A Novel PET Agent for In Vivo Detection of Dense Amyloid Plaques in Alzheimer's Disease Patients. J Nucl Med.